# P^2^,P^3^-[^18^F]Monofluoromethylene diadenosine-5’,5’’’-P^1^,P^4^-tetraphosphate

Chemical name: | P^2^, P^3^-[^18^F]Monofluoromethylene diadenosine-5’,5’’’-P^1^,P^4^-tetraphosphate
Abbreviated name: | [^18^F]AppCHFppA
Synonym:
Agent category: | Small molecule
Target: | Adenosine nucleotide receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal/contrast: | ^18^F
Activation: | No
Studies: | - Rodents; - Non-primate non-rodent mammals | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F + Ap2CHFp2A)]

Extracellular adenine 5’-diphosphates (ADP) are released from a variety of cells and regulate many physiological processes by interacting with purine receptors or adenosine receptors (1). In particular, high concentrations of ADP are built up in atherosclerotic lesions, where they either inhibit platelet aggregation via binding to platelet receptors (P2T) and/or accumulate in macrophages, monocytes, and smooth muscle cells via binding to purine receptors (P2X and P2Y) (2, 3). Diadenosine oligophosphate (Ap4A), a nucleotide oligomer made from two adenosine moieties joined in 5’-5’ linkage by a tetraphosphodiester linkage (4), is a competitive inhibitor of ADP in platelet aggregation (5, 6). Because platelet aggregation plays a central role in arterial thrombosis and plaque formation, Ap4A was initially proposed as a therapeutic agent for inhibition and treatment of plaque formation (1). However, Ap4A has a short blood half-life due to the rapid degradation by phosphodiesterase (5). A series of analogs are synthesized by substituting the oxygen bridge in the β,β’ position of Ap4A with -CHX- to produce β,β’-monohalomethylene diadenosine 5’,5’’’-P^1^,P^4^-tetraphosphate (AppCHXppA, X=Cl, F) (6). This modification increases its resistance to hydrolytic enzymes and generates a potent antithrombotic agent (6). For instance, AppCHFppA can effectively inhibit ADP-induced platelet aggregation with a 4 μM of half maximal (50%) inhibitory concentration (5).

[^18^F]AppCHFppA is an ^18^F-labeled molecular probe for positron emission tomography (PET) (7). ^18^F has a half-life of 109.8 min, an ideal radionuclide for routine PET imaging (8). The low β^+^ energy of ^18^F provides a short positron linear range in tissues and particularly high resolution in PET imaging (8). [^18^F]AppCHFppA can accumulate selectively in atherosclerotic lesions, which allows noninvasive characterization of plaque inflammation with PET imaging (7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F + Ap2CHFp2A)+AND+synthesis%0D%0A)]

[^18^F]AppCHFppA was obtained through a multi-step synthesis (7). First, the precursor AppCHClppA was produced by condensation of AMP, dAMP, ADP, and deoxyadenosine 5’-thiophosphate with monochloromethylene or bismonochloromethylene triphosphonate in the presence of diphenyl phosphochloridate (9). AppCHClppA was converted to tributylammonium salts, which dissolve in organic solvents, and then it was reacted with [^18^F]fluoride (3.7 GBq (100 mCi)) by nucleophilic substitution (7). The produced [^18^F]AppCHFppA had a yield of 20–40% and a radiochemical purity of 98% (specific activity >185,000 GBq/mmol (5,000 Ci/mmol)) for injection.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F+ Ap2CHFp2A)+AND+%22in+vitro%22)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F+ Ap2CHFp2A) +AND++rodentia)]

Elmaleh et al. performed a biodistribution study of [^18^F]AppCHFppA in rats (300–350 g) (7). After administration of [^18^F]AppCHFppA (185 MBq/kg body weight), animals were euthanized. Tissue samples were collected, and radioactivity was measured with a gamma counter. [^18^F]AppCHFppA exhibited typical ADP behavior in normal rats and had significant myocardial uptake and fast kidney clearance. The accumulation (percentage of injected dose per gram (% ID/g)) in most tissues was measured at 5, 30, and 60 min: blood (0.78, 0.16, and 0.07), heart (0.33, 0.08, and 0.03), lung (0.62, 0.18, and 0.08), liver (0.33, 0.08, and 0.03), and kidney (2.10, 0.90, and 0.03). Bone demonstrated some accumulation (1.04, 1.51, and 1.83) as a result of defluorination and/or tetraphosphonate bone uptake. Of all the tissue samples, the kidney contained the highest early concentration of tracer, the liver and lung had higher concentrations than the spleen and muscle, and the spleen accumulation was similar to that in muscle. No metabolized rate was reported for AppCHFppA.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Elmaleh et al. used [^18^F]AppCHFppA to examine atherosclerotic lesions in rabbits (2.5–3.0 kg) (7). After induction injury to the aorta, the rabbits were maintained on a high-cholesterol diet for 3–6 months to achieve atherosclerosis and inflammation. MicroPET imaging was performed after intravenous injection of [^18^F]AppCHFppA (118 MBq). The images demonstrated a rapid accumulation of [^18^F]AppCHFppA in the atherosclerotic abdominal aorta. The atherosclerotic lesions were clearly visible 10 min after injection and retained through the 1-h imaging session. During the imaging study, blood was sampled at 1–40 min to evaluate blood clearance of [^18^F]AppCHFppA. The lesion/blood radioactivity ratio was >5:1 at 1 h. After the imaging experiment, small sections were extracted from both lesional and normal aortic segments (aortic and iliac specimens) for histological examination. The [^18^F]AppCHFppA uptake measured by PET was well correlated with the immunostaining of plaque macrophage density.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F + Ap2CHFp2A) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F +- Ap2CHFp2A) +AND+human)]

No publication is currently available.

### NIH Support

AI060872

## References

1 Elmaleh D.R., Narula J., Babich J.W., Petrov A., Fischman A.J., Khaw B.A., Rapaport E., Zamecnik P.C. (1998). Rapid noninvasive detection of experimental atherosclerotic lesions with novel 99mTc-labeled diadenosine tetraphosphates. Proc Natl Acad Sci U S A.
2 Kunapuli S.P. (2002). P2 receptors and platelet activation. ScientificWorldJournal.
3 Murugappa S., Kunapuli S.P. (2006). The role of ADP receptors in platelet function. Front Biosci.
4 Kisselev L.L., Justesen J., Wolfson A.D., Frolova L.Y. (1998). Diadenosine oligophosphates (Ap(n)A), a novel class of signalling molecules?. FEBS Lett.
5 Zamecnik P.C., Kim B., Gao M.J., Taylor G., Blackburn G.M. (1992). Analogues of diadenosine 5',5'''-P1,P4-tetraphosphate (Ap4A) as potential anti-platelet-aggregation agents. Proc Natl Acad Sci U S A.
6 Kim B.K., Zamecnik P., Taylor G., Guo M.J., Blackburn G.M. (1992). Antithrombotic effect of beta,beta'-monochloromethylene diadenosine 5',5"'-P1,P4-tetraphosphate. Proc Natl Acad Sci U S A.
7 Elmaleh D.R., Fischman A.J., Tawakol A., Zhu A., Shoup T.M., Hoffmann U., Brownell A.L., Zamecnik P.C. (2006). Detection of inflamed atherosclerotic lesions with diadenosine-5',5'''-P1,P4-tetraphosphate (Ap4A) and positron-emission tomography. Proc Natl Acad Sci U S A.
8 Wester H.J., Schottelius M., Scheidhauer K., Meisetschlager G., Herz M., Rau F.C., Reubi J.C., Schwaiger M. (2003). PET imaging of somatostatin receptors: design, synthesis and preclinical evaluation of a novel 18F-labelled, carbohydrated analogue of octreotide. Eur J Nucl Med Mol Imaging.
9 Chan S.W., Gallo S.J., Kim B.K., Guo M.J., Blackburn G.M., Zamecnik P.C. (1997). P1,P4-dithio-P2,P3-monochloromethylene diadenosine 5',5'''-P1,P4-tetraphosphate: a novel antiplatelet agent. Proc Natl Acad Sci U S A.